# ^18^F-Labeled fluoropegylated 6-fluoroethoxy-4'-dimethylaminoflavone, 6-(2-(2-fluoro-ethoxy)-ethoxy)-4'-dimethylaminoflavone, and 6-(2-(2-(2-fluoro-ethoxy)-ethoxy)ethoxy)-4'-dimethylaminoflavone

Chemical name: | ^18^F-Labeled fluoropegylated 6-fluoroethoxy-4'-dimethylaminoflavone, 6-(2-(2-fluoro-ethoxy)-ethoxy)-4'-dimethylaminoflavone, and 6-(2-(2-(2-fluoro-ethoxy)-ethoxy)ethoxy)-4'-dimethylaminoflavone | [image]
Abbreviated name: | [^18^F]8(a–c) | [image]
Synonym: | [^18^F]8a, [^18^F]8b, [^18^F]8c | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) | [image]
Target Category: | Accepters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]8(a–c) by Ono et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20)]

^18^F-Labeled fluoropegylated 6-fluoroethoxy-4'-dimethylaminoflavone (compound 8a), 6-(2-(2-fluoro-ethoxy)-ethoxy)-4'-dimethylaminoflavone (compound 8b), and 6-(2-(2-(2-fluoro-ethoxy)-ethoxy)ethoxy)-4'-dimethylaminoflavone (compound 8c), abbreviated as [^18^F]8a, [^18^F]8b, and [^18^F]8c, respectively, are flavone derivatives synthesized by Ono et al. for positron emission tomography (PET) of Alzheimer’s disease (AD) by targeting β-amyloid (Aβ) (1).

AD is characterized in pathology by the presence of extracellular Aβ plaques, intraneuronal neurofibrillary tangles, and neuronal loss in the cerebral cortex (2, 3). Of them, Aβ deposit is the earliest neuropathological marker and is relatively specific to AD and closely related disorders. Aβ plaques are composed of abnormal paired helical filaments 5–10 nm in size. These filaments are largely made of insoluble Aβ peptides that are 40 or 42 amino acids in length (4).

In recent years, molecular imaging by targeting the extracellular Aβ has been intensively investigated in attempts to detect early AD, assess Aβ content in vivo, determine the timing of anti-plaque therapy, and evaluate the therapeutic efficacy (4). Radiolabeled Aβ40 peptides were tested first, but they showed poor penetration ability to cross the blood–brain barrier (BBB) (4). Based on the fact that Aβ can be specifically stained in vitro with dyes of Congo red, chrysamine G, and thioflavin-T, an effort was made to develop imaging agents with these dyes. This effort, however, was in general unsuccessful because the bulky ionic groups of heteroatoms in these dyes prevent them from crossing the BBB (2). Importantly, a large class of derivatives (e.g., aminonaphthalenes, benzothiazoles, stilbenes, and imidazopyridines) was synthesized with these dyes as templates (4). Clinical and preclinical studies have shown that these derivatives not only possess a high binding affinity with Aβ plaques as their parent compounds, but also exhibit good penetration ability through the BBB and rapid washout from brain with low to no plaque deposits.

Ono et al. first synthesized a class of radioiodinated flavone derivatives that present a high binding affinity with Aβ plaques and good penetration ability through the BBB (5). However, these flavone derivatives display poor clearance from the brain, which leads to a high brain background. The investigators then explored another class of flavonoids with aurone as the core structure (1, 6). Aurone is a heterocyclic chemical compound that contains a benzofuran element associated with a benzylidene linked in position 2 and a chalcone-like group being closed into a five-member ring. The aurone derivatives possess a nucleophilic group (NH_2_, NHMe, or NMe_2_) at the 4' position and a radioiodine at the 5 position. Although these aurone derivatives exhibit a strong binding affinity with Aβ (inhibition constant (K_i_) = 1.2–6.8 nM), high penetration ability through the BBB (1.9%−4.6% injected dose per gram tissue (ID/g) at 2 min), and a fast washout from the brain (0.3%−0.5% ID/g at 30 min), the pharmacokinetics of these compounds are less favorable for brain imaging than the pharmacokinetics of the agent [^123^I]IMPY (6-iodo-2-(4'-dimethylamino)phenyl-imidazo[1,2]pyridine), which is the only SPECT agent to be tested in humans to date (7-9). The investigators also modified the flavone and aurone derivatives by pegylating them with 1–3 units of ethylene glycol at the 4' position or by conjugating them with the chelating agent bis-amino-bis-thiol (BAT). Favorable pharmacokinetics for brain imaging was observed for the pegylated derivatives ([^18^F]8(a–c)) but not for the BAT-chelated derivatives ([^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR) (1, 6).

This series of chapters summarizes the data obtained with flavone and aurone derivatives, including [^125^I]15, [^125^I]9, [^125^I]14, [^125^I]16, [^125^I]17, [^99m^Tc]BAT-FL, [^99m^Tc]BAT-AR, [^18^F]8(a–c), [^125^I]3, and [^18^F]3 (1, 6-8). This chapter presents the data obtained with [^18^F]8(a–c) (1).

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=19201614)]

The synthesis of the compound precursors with chemical yields was described in detail by Ono et al. (1). [^18^F]8(a–c) was obtained with the reaction of the corresponding tosylate precursors with [^18^F]fluoride. The reaction mixture was purified with reversed phase high-performance liquid chromatography. The radiochemical purities of the final products were >99%; radiochemical yields ranged from 5% to 13%; total synthesis times were 70 min; and specific activities were 33.3–55.5 GBq/mmol (900–1,500 mCi/mmol) at the end of synthesis.

[^125^I]6-Iodo-4'-dimethylaminoflavone ([^125^I]DMFV, K_d_ = 12.3 nM) was prepared as the radioligand in binding assays using the standard iododestannylation reaction (10). The specific activity and radiochemical purity of [^125^I]DMFV were 81.4 TBq/mmol (2.2 kCi/mmol) and >95%, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=19201614)]

The binding of [^18^F]8(a–c) with Aβ aggregates was carried out with [^125^I]DMFV in solutions (1, 10). The K_i_ values were measured to be 5.3, 14.4, and 19.3 for [^18^F]8a, [^18^F]8b, and [^18^F]8c, respectively. The results of K_i_ measurement for [^18^F]8(a–c) and other derivatives indicate that the affinities of flavone derivatives for Aβ(1–42) aggregates were affected by the group substituted at the 4' position in the flavone structure, not by the length of ethylene glycol introduced into the flavone backbone (1).

The affinity of [^18^F]8(a–c) for brain Aβ plaques was analyzed with brain sections of Tg2576 transgenic mice with fluorescence staining (1). Many fluorescent spots were observed, and these findings were consistent with those obtained with immunohistochemical labeling with an antibody specific for Aβ. No spots were observed in the brain sections of wild-type mice (data not shown). These results indicate that [^18^F]8(a–c) can bind specifically with Aβ plaques in the mouse brain.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=19201614)]

The biodistribution of [^18^F]8(a–c) was examined in normal mice (n = 4–5/time point for each agent) (1). All three ligands displayed high radioactivity in the brain at 2 min after injection (2.89%–4.17% ID/g). Low radioactivity was observed at 30 min after injection (1.89%, 2.00%, and 1.31% ID/g for [^18^F]8a, [^18^F]8b, and [^18^F]8c, respectively). These values were equal to 45.3%, 56.5%, and 45.3% of the initial uptake peak for [^18^F]8a, [^18^F]8b, and [^18^F]8c, respectively, indicating a rapid initial uptake in normal brain tissue coupled with a fast washout, which is highly desirable for Aβ imaging. [^18^F]8(a–c) also showed high bone uptake (3.74%–6.21% ID/g) at 60 min after injection, suggesting there may be in vivo defluorination. However, the interference from this free fluoride is expected to be relatively low for brain imaging because the free fluorine was not taken up by brain tissue (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Ono M., Watanabe R., Kawashima H., Kawai T., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). 18F-labeled flavones for in vivo imaging of beta-amyloid plaques in Alzheimer's brains. Bioorg Med Chem.
2 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
3 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
4 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
5 Ono M., Maya Y., Haratake M., Ito K., Mori H., Nakayama M. (2007). Aurones serve as probes of beta-amyloid plaques in Alzheimer's disease. Biochem Biophys Res Commun.
6 Ono M., Ikeoka R., Watanabe H., Kimura H., Fuchigami T., Haratake M., Saji H., Nakayama M. (2010). 99mTc/Re complexes based on flavone and aurone as SPECT probes for imaging cerebral beta-amyloid plaques. Bioorg Med Chem Lett.
7 Maya Y., Ono M., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). Novel radioiodinated aurones as probes for SPECT imaging of beta-amyloid plaques in the brain. Bioconjug Chem.
8 Watanabe H., Ono M., Kimura H., Kagawa S., Nishii R., Fuchigami T., Haratake M., Nakayama M., Saji H. (2011). A dual fluorinated and iodinated radiotracer for PET and SPECT imaging of beta-amyloid plaques in the brain. Bioorg Med Chem Lett.
9 Newberg A.B., Wintering N.A., Plossl K., Hochold J., Stabin M.G., Watson M., Skovronsky D., Clark C.M., Kung M.P., Kung H.F. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.
10 Ono M., Yoshida N., Ishibashi K., Haratake M., Arano Y., Mori H., Nakayama M. (2005). Radioiodinated flavones for in vivo imaging of beta-amyloid plaques in the brain. J Med Chem.